# Vascular endothelial growth factor A isoform 121-gelonin fusion protein–conjugated manganese ferrite nanoparticles

Chemical name: | Vascular endothelial growth factor A isoform 121-gelonin fusion protein–conjugated manganese ferrite nanoparticles
Abbreviated name: | VEGF_121_/rGel-MNPs
Synonym:
Agent Category: | Nanoparticles
Target: | Vascular endothelial growth factor receptor (VEGFR)
Target Category: | Receptors
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Manganese ferrite (MnFe_2_O_4_)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=antiangiogenic%20therapy%20and%20VEGFR%20and%20VEGF)]

The vascular endothelial growth factor A isoform 121 (VEGF_121_)-gelonin fusion protein (VEGF_121_/rGel)–conjugated manganese ferrite (MnFe_2_O_4_) nanoparticle (NP), abbreviated as VEGF_121_/rGel-MNP, is a VEGF receptor (VEGFR)-targeted contrast agent developed by Cho et al. for monitoring the targeting efficiency and treatment efficacy of the VEGF_121_/rGel immunotoxin (1).

VEGFs are a group of five potent inducers of cell migration, invasion, vascular permeability, and neovascular formation (2). They act via three receptor tyrosine kinases: VEGFR-1, VEGFR-2, and VEGFR-3 (3). These receptors are overexpressed on the endothelial cells of tumor neovasculature and are almost undetectable in the endothelium of adjacent normal tissues. The critical role of the VEGF/VEGFR signal pathway in tumor angiogenesis has prompted great efforts in the development of antiangiogenic therapies, and agents have been tested by acting on different steps of the pathway, such as by binding to the VEGF ligand, inhibiting VEGFR tyrosine kinase, inhibiting downstream effectors (mammalian target of rapamycin inhibitors), and modulating VEGF production (4-6). These agents are highly effective against tumor growth in animal models when they are used alone; however, they seldom lead to tumor regression and exhibit insufficient efficacy in the clinical setting, although combination with chemotherapy has been shown to improve patient survival in certain tumor types. The most likely explanation for this phenominon is that tumor endothelial cells can adapt to antiangiogenic treatment and form functional vasculature that loses sensitivity to the inhibitors of VEGF/VEGFR (4, 6). It is hypothesized that VEGF/VEGFR-targeted therapy should be administrated before the development of a well-established vascular network.

Molecular imaging provides a means to reveal the mechanism underlying this phenomenon and to monitor the antiangionic therapy (1, 7). VEGF_121_/rGel has been generated with VEGF_121_, which is linked with recombinant plant toxin gelonin through a G_4_S tether (4, 8-10). Gelonin is a member of the ribosome-inactivating protein family, which depurinates rRNA and other polynucleotide substrates and subsequently inhibits protein synthesis (7, 11). A series of preclinical studies showed that VEGF_121_/rGel could specifically inhibit the growth of tumor endothelial cells (8-10, 12). Like other immunotoxins, VEGF_121_/rGel is also expected to be effective against tumors resistant to VEGF/VEGFR-targeting inhibitors if the tumor cells express sufficient levels of VEGFR. To monitor the VEGFR-targeting efficiency of VEGF_121_/rGel with imaging techniques, Hsu et al. and Cho et al. labeled the VEGF_121_/rGel with ^64^Cu (^64^Cu-DOTA-VEGF_121_/rGel) and with MnFe_2_O_4_ NPs (VEGF_121_/rGel-MNPs), respectively (1, 7). Both imaging studies have concluded that noninvasive imaging with VEGF_121_/rGel will be useful to monitor the treatment efficacy and to identify patients who may benefit from the VEGF_121_/rGel therapy. This chapter summarizes data obtained with VEGF_121_/rGel-MNPs.

### Related Resource Links:

VEGF/VEGFR-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=VEGFR%20AND%20micad%5bbook%5d)

Articles on VEGF in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim?term=vascular%20endothelial%20growth%20factor)

VEGF-related compounds in PubChem Substance (http://www.ncbi.nlm.nih.gov/pcsubstance?term=vascular%20endothelial%20growth%20factor)

VEGF-related nucleotide sequences (http://www.ncbi.nlm.nih.gov/nuccore?term=VEGF)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21512397)]

Cho et al. described the synthesis of VEGF_121_/rGel-MNPs (1). MnFe_2_O_4_ NPs (diameter, ~12 nm) were synthesized with the seed-mediated growth method and capped with carboxylated polysorbate 80 to generate carboxylated water-soluble NPs. Characterization showed that the NPs exhibited superparamagnetic behavior without magnetic hysteresis, had a saturation magnetization value of 1.56 emu/g at 0.85 T, and had a relaxivity coefficient of 423 mM−^1^s−^1^ at 1.5 T. The size of the NPs was determined with light scattering to be 38.9 ± 0.6 nm. The colloidal stability was maintained for >3 months.

The synthesis, expression, and purification of the VEGF_121_/rGel immunotoxin were performed as described previously by Veenendaal et al. (8). The molecular weight of VEGF_121_/rGel was 84 kDa. VEGF_121_/rGel was conjugated to the carboxyl group of the carboxylated NPs. Conjugation of the VEGF_121_/rGel to the NPs increased the NP size slightly to 44.5 ± 1.2 nm and changed the surface charge from −19.6 ± 3.1 mV to −1.4 ± 3.9 mV. There were ~17 equivalent VEGF_121_/rGel molecules per carboxylated NP.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21512397)]

Cho et al. first evaluated the expression levels of a set of receptors in a group of cell lines (1). PAE/KDR cells (porcine aortic endothelial cells transfected with cDNA of VEGFR2) exhibited >105 times and >108 times more VEGFR2 expression than did HUVEC cells and 253JB-V cells (a human bladder cancer cell line), respectively. The binding of VEGF_121_/rGel-MNPs with VEGFR2 was tested using PAE/KDR cells that overexpress VEGFR2, with 253JB-V cells as the control. T2-Weighted magnetic resonance imaging (MRI) at 1.5 T showed that VEGF_121_/rGel-MNPs exhibited a dose-dependent enhancement of the signal intensity over the concentration range of 0.04–5.0 µg for the PAE/KDR cells but not for the 253JB-V cells. VEGF_121_/rGel-MNPs were predominantly localized in the cytoplasm.

The binding specificity of VEGF_121_/rGel-MNPs to PAE/KDR cells was further tested with VEGF_121_ as a competeting inhibitor (1). PAE/KDR cells were pretreated for 1 h at 4°C with VEGF_121_ (molar ratios of 0.1, 1.0, and 10.0 compared with equivalent VEGF_121_/rGel). Cells were then incubated with 3.0 µg VEGF_121_/rGel-MNPs for 1 h. As the molar ratio of VEGF_121_:VEGF_121_/rGel increased, the signal enhancement decreased. At a molar ratio of 10.0, the normalized ΔR2/R2_noninhibition_ value was ~90%.

The biological activity of the VEGF_121_/rGel-MNPs on VEGFR2 expression after incubation with PAE/KDR cells for 72 h at 37°C was analyzed with immunoblotting (1). The expression of phosphorylated VEGFR2 was slightly reduced with VEGF_121_/rGel-MNPs compared with VEGF_121_/rGel, but increased expression was observed at concentrations ≥10 nM. The 50% inhibition concentrations of free VEGF_121_/rGel, rGel, and VEGF_121_/rGel-MNPs on PAE/KDR cells after 72 h incubation were determined to be 0.4, 76.1, and 50.3 nM, respectively..

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21512397)]

In vivo MRI was performed in male BALB/c nude mice bearing 253JB-V tumor xenografts in the bladder dome (n = 5 mice) (1). VEGF_121_/rGel-MNPs (200 µg Fe + Mn/200 µl) were injected via the tail vein, and MRI was performed at 3.0 T. After injection, MRI signal enhancement was identified initially for the vessels surrounding the bladder and later for the intratumoral vessels (for up to 4 h). Pretreatment with VEGF_121_ (200 µg Fe) for 4 h blocked the contrast enhancement of tumor vessels induced by VEGF_121_/rGel-MNPs, showing significant enhancement of the tumor vessels immediatelty after VEGF_121_/rGel-MNPs injection which was then disappeared within 4 h. These results were confirmed with ex vivo images. The targeted delivery of VEGF_121_/rGel-MNPs to intratumoral vessels was further verified with immunofluorescence staining of the gelonin and endothelial cells.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Cho E.J., Yang J., Mohamedali K.A., Lim E.K., Kim E.J., Farhangfar C.J., Suh J.S., Haam S., Rosenblum M.G., Huh Y.M. (2011). Sensitive Angiogenesis Imaging of Orthotopic Bladder Tumors in Mice Using a Selective Magnetic Resonance Imaging Contrast Agent Containing VEGF121/rGel. Invest Radiol.
2 Koch S., Tugues S., Li X., Gualandi L., Claesson-Welsh L. (2011). Signal transduction by vascular endothelial growth factor receptors. Biochem J.
3 Press M.F., Lenz H.J. (2007). EGFR, HER2 and VEGF pathways: validated targets for cancer treatment. Drugs.
4 Backer M.V., Hamby C.V., Backer J.M. (2009). Inhibition of vascular endothelial growth factor receptor signaling in angiogenic tumor vasculature. Adv Genet.
5 Munagala R., Aqil F., Gupta R.C. (2011). Promising molecular targeted therapies in breast cancer. Indian J Pharmacol.
6 Thorpe P.E. (2004). Vascular targeting agents as cancer therapeutics. Clin Cancer Res.
7 Hsu A.R., Cai W., Veeravagu A., Mohamedali K.A., Chen K., Kim S., Vogel H., Hou L.C., Tse V., Rosenblum M.G., Chen X. (2007). Multimodality molecular imaging of glioblastoma growth inhibition with vasculature-targeting fusion toxin VEGF121/rGel. J Nucl Med.
8 Veenendaal L.M., Jin H., Ran S., Cheung L., Navone N., Marks J.W., Waltenberger J., Thorpe P., Rosenblum M.G. (2002). In vitro and in vivo studies of a VEGF121/rGelonin chimeric fusion toxin targeting the neovasculature of solid tumors. Proc Natl Acad Sci U S A.
9 Mohamedali K.A., Kedar D., Sweeney P., Kamat A., Davis D.W., Eve B.Y., Huang S., Thorpe P.E., Dinney C.P., Rosenblum M.G. (2005). The vascular-targeting fusion toxin VEGF121/rGel inhibits the growth of orthotopic human bladder carcinoma tumors. Neoplasia.
10 Akiyama H., Mohamedali K.A. (2005). E.S. RL, S. Kachi, J. Shen, C. Hatara, N. Umeda, S.F. Hackett, S. Aslam, M. Krause, H. Lai, M.G. Rosenblum, and P.A. Campochiaro, Vascular targeting of ocular neovascularization with a vascular endothelial growth factor121/gelonin chimeric protein. Mol Pharmacol.
11 Wahl O., Oswald M., Tretzel L., Herres E., Arend J., Efferth T. (2011). Inhibition of tumor angiogenesis by antibodies, synthetic small molecules and natural products. Curr Med Chem.
12 Ran S., Mohamedali K.A., Luster T.A., Thorpe P.E., Rosenblum M.G. (2005). The vascular-ablative agent VEGF(121)/rGel inhibits pulmonary metastases of MDA-MB-231 breast tumors. Neoplasia.